# 1-(9H-Carbazol-4-yloxy)-3-(2-(2-[^11^C]methoxyphenoxy)ethylamino)-propan-2-ol

Chemical name: | 1-(9H-Carbazol-4-yloxy)-3-(2-(2-[^11^C]methoxyphenoxy)ethylamino)-propan-2-ol
Abbreviated name: | [^11^C]CARV
Synonym: | [^11^C]Carvedilol
Agent category: | Compound
Target: | P-glycoprotein multidrug transporter, MDR-1
Target category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=carvedilol%20and%2011C)]

One of the mechanisms cells use to escape the cytotoxic effects of chemotherapeutic agents, such as Adriamycin, Vinca alkaloids, epipodophyllotoxins, actinomycin D, and Taxol_,_ is to limit their presence inside the cells through the actions of P-glycoprotein (P-gp), a protein encoded by the multidrug resistance (MDR-1) gene (1, 2). P-gp is an ATP-dependent transmembrane multidrug transporter that is capable of actively pumping a variety of agents out of cells. Overexpression of P-gp in tumor cells (such as renal carcinoma, hepatoma, pheochromocytoma, and colon carcinoma) leads to resistance to anticancer drugs (3). P-gp is also present in a variety of normal cells, such as intestinal mucosal cells, hepatocytes, renal proximal tubule epithelial cells, and endothelial cells of the blood-brain barrier (4, 5). Calcium channel blockers, cyclosporin A, and its non-immunosuppressive analog PSC 833 are MDR modulators that inhibit transport of P-gp substrates out of cells (6, 7).

Sestamibi (MIBI) is a substrate for P-gp. ^99m^Tc-MIBI has been approved by the United States Food and Drug Administration as a myocardial perfusion imaging agent for use in single-photon emission computed tomography (SPECT) to assess the risk of future cardiac events. It is also approved as a tumor-imaging agent in breast, lung, thyroid, and brain cancers. 1-(9H-Carbazol-4-yloxy)-3-[2-(2-methoxyphenoxy)ethylamino]-propan-2-ol (carvedilol), a β-adrenoceptor antagonist, is also a transport substrate for P-gp with a log P of 2.0 (8). [^11^C]Carvedilol ([^11^C]CARV) was found to be not suitable as a tracer for imaging adrenoceptors in any target organ, such as the brain, heart, lungs, and spleen (9). Brain accumulation of [^11^C]CARV is reported to be highly sensitive to P-gp modulation by cyclosporin A (10). Therefore, [^11^C]CARV is being developed as a positron emission tomography (PET) agent to noninvasively study P-gp function.

### Related Resource Links:

- Chapters in MICAD (P-glycoprotein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (P-glycoprotein (http://www.ncbi.nlm.nih.gov/gene/5243))
- Articles in OMIM (P-glycoprotein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=P-glycoprotein%5BAll+Fields%5D))
- Clinical trials (P-glycoprotein (http://www.clinicaltrials.gov/ct2/results?term=P-glycoprotein), ^99m^Tc-MIBI (http://www.clinicaltrials.gov/ct2/results?term=Sestamibi), Carvedilol (http://www.clinicaltrials.gov/ct2/results?term=Carvedilol))
- Drug information in FDA (^99m^Tc-MIBI (http://google2.fda.gov/search?q=99mTc-sestamibi+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=16), Carvedilol (http://google2.fda.gov/search?q=Carvedilol&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=carvedilol%2011C%20and%20synthesis)]

In the report by Bart et al. (10), [^11^C]CARV was synthesized by alkylation of desmethylcarvedilol with [^11^C]methyltriflate, with subsequent separation by high-performance liquid chromatography. The radiochemical yield was 20-33%, based on [^11^C]methyltriflate, with a total synthesis time of 55 min. The specific activity was 13-26 TBq/mmol (350-703 Ci/mmol) at the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=carvedilol%2011C%20and%20cells)]

In a study using the P-gp-negative small cell lung carcinoma GLC_4_ and its overexpressing subclone GLC_4_/P-gp, cellular accumulation of [^11^C]CARV was 100% higher in GLC_4_ than in GLC_4_/P-gp (10). Cyclosporin A (50 μM) increased [^11^C]CARV accumulation by 2.0-fold (P = 0.0001) in GLC_4_/P-gp but had no effect in GLC_4_. MK571 (50 μM), a multidrug resistance-associated protein (MRP1) inhibitor, had no effect on [^11^C]CARV accumulation in both cell types.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=carvedilol%2011C%20and%20rodentia)]

Biodistribution studies in normal rats showed high accumulation of radioactivity, as measured by autoradiography, in the lung, followed by the liver, kidney, and heart at 60 min after injection of [^11^C]CARV (10). Tracer accumulation in the brain was low. Cyclosporin A (25-50 mg/kg) increased [^11^C]CARV accumulation in the brain 6 ± 3-fold. This indicates that P-gp-mediated [^11^C]CARV efflux can be modulated by cyclosporin A. PET imaging revealed that [^11^C]CARV accumulated in the brains of rats without or with cyclosporin A treatment (5, 10, 15, 25, and 50 mg/kg). The tracer was rapidly cleared from plasma after injection, with a first phase half-life of 2.3 min and a second, wash-out phase half-life of 108 min. Cyclosporin A had no effects on the plasma kinetics of [^11^C]CARV. The distribution volume (DV) of [^11^C]CARV in the brain was 0.3 after injection of 35-50 MBq (0.94-1.35 mCi) of [^11^C]CARV. At 5 mg/kg cyclosporin A, the DV was increased >1-fold. The maximum increase in DV was 2-fold after 15 mg/kg cyclosporin A with no further increases at higher dosages of cyclosporin A. Metabolism studies using [^14^C]CARV in rats, mice, and dogs showed that all metabolites are more hydrophilic than the parent compound and are expected to have negligible brain uptake (11).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28carvedilol%20carbon%20radioisotopes%29%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No relevant publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28carvedilol%20carbon%20radioisotopes%29%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28carvedilol%20carbon%20radioisotopes%29%20and%20human)]

No relevant publications are currently available.

## References

1 Endicott J.A., Ling V. (1989). The biochemistry of P-glycoprotein-mediated multidrug resistance. Annu Rev Biochem.
2 Gottesman M.M., Pastan I. (1993). Biochemistry of multidrug resistance mediated by the multidrug transporter. Annu Rev Biochem.
3 Fojo A.T., Ueda K., Slamon D.J., Poplack D.G., Gottesman M.M., Pastan I. (1987). Expression of a multidrug-resistance gene in human tumors and tissues. Proc Natl Acad Sci U S A.
4 Piwnica-Worms D., Rao V.V., Kronauge J.F., Croop J.M. (1995). Characterization of multidrug resistance P-glycoprotein transport function with an organotechnetium cation. Biochemistry.
5 Thiebaut F., Tsuruo T., Hamada H., Gottesman M.M., Pastan I., Willingham M.C. (1987). Cellular localization of the multidrug-resistance gene product P-glycoprotein in normal human tissues. Proc Natl Acad Sci U S A.
6 Hughes C.S., Vaden S.L., Manaugh C.A., Price G.S., Hudson L.C. (1998). Modulation of doxorubicin concentration by cyclosporin A in brain and testicular barrier tissues expressing P-glycoprotein in rats. J Neurooncol.
7 Mayer U., Wagenaar E., Dorobek B., Beijnen J.H., Borst P., Schinkel A.H. (1997). Full blockade of intestinal P-glycoprotein and extensive inhibition of blood-brain barrier P-glycoprotein by oral treatment of mice with PSC833. J Clin Invest.
8 Jonsson O., Behnam-Motlagh P., Persson M., Henriksson R., Grankvist K. (1999). Increase in doxorubicin cytotoxicity by carvedilol inhibition of P-glycoprotein activity. Biochem Pharmacol.
9 Doze P., Elsinga P.H., Maas B., Van Waarde A., Wegman T., Vaalburg W. (2002). Synthesis and evaluation of radiolabeled antagonists for imaging of beta-adrenoceptors in the brain with PET. Neurochem Int.
10 Bart J., Dijkers E.C., Wegman T.D., de Vries E.G., van der Graaf W.T., Groen H.J., Vaalburg W., Willemsen A.T., Hendrikse N.H. (2005). New positron emission tomography tracer [(11)C]carvedilol reveals P-glycoprotein modulation kinetics. Br J Pharmacol.
11 Schaefer W.H., Politowski J., Hwang B., Dixon F., Goalwin A., Gutzait L., Anderson K., DeBrosse C., Bean M., Rhodes G.R. (1998). Metabolism of carvedilol in dogs, rats, and mice. Drug Metab Dispos.